# ^64^Cu-1,4,7-Triazacyclononane-1,4-diacetic acid-6-aminohexanoic acid-Gln-Trp-Ala-Val-Gly-His-Leu-Met-NH_2_

Chemical name: | ^64^Cu-1,4,7-Triazacyclononane-1,4-diacetic acid-6-aminohexanoic acid-Gln-Trp-Ala-Val-Gly-His-Leu-Met-NH_2_ | [image]
Abbreviated name: | ^64^Cu-NO2A-(6-Ahx)-BBN(7–14)NH_2_ | [image]
Synonym: | ^64^Cu-NO2A-(X)-BBN(7–14)NH_2_ | [image]
Agent Category: | Peptides | [image]
Target: | Gastrin-releasing peptide receptors (GRPR) | [image]
Target Category: | Receptors | [image]
Method of detection: | Positron emission tomography (PET) | [image]
Source of signal / contrast: | ^64^Cu | [image]
Activation: | No | [image]
Studies: | - In vitro; - Rodents | Structure of Cu-NO2A-(6-Ahx)-BBN(7-14)NH_2_ by Lane et al (1).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=GRPR+and+bombesin+and+imaging)]

^64^Cu-1,4,7-Triazacyclononane-1,4-diacetic acid (NO2A)-6-aminohexanoic acid (6-Ahx)-Gln-Trp-Ala-Val-Gly-His-Leu-Met-NH_2_ (BBN(7–14)NH_2_), abbreviated as ^64^Cu-NO2A-(6-Ahx)-BBN(7–14)NH_2_, is a bombesin (BBN)-based, ^64^Cu-NO2A-conjugated peptide that was synthesized by Lane et al. for use in positron emission tomography (PET) of tumors expressing gastrin-releasing peptide receptor (GRPR) (1, 2).

GRPR is a glycosylated G-protein–coupled receptor that is normally expressed in non-neuroendocrine tissues of the breast and pancreas and in neuroendocrine cells of the brain, gastrointestinal tract, lung, and prostate (3, 4). GRPR has been found to be overexpressed in various human tumors, and a large number of BBN analogs have been investigated for GRPR-targeted imaging and therapy (5, 6). These analogs have been synthesized on the basis of either truncated BBN (BBN(6–14) or BBN(7–14)) or full-length BBN(1–14) (7, 8). Chelators and spacers have been used frequently for chelating metals and for improving the kinetics of conjugates (9-11).

^64^Cu is a radiometal with potential applications in diagnostic and therapeutic nuclear medicine. The half-life for ^64^Cu (t_1/2_ = 12.7 h) is long enough for drug preparation, quality control, imaging, and therapy (12, 13). However, use of ^64^Cu is limited by issues of in vivo transchelation to proteins found in blood and liver (such as superoxide dismutase) (1). A variety of chelators have been investigated for the purpose of stably chelating ^64^Cu (13). In general, ^64^Cu-labeled 1,4,7,10-tetraazacyclodecane-1,4,7,10-tetraacetic acid (^64^Cu-DOTA) and ^64^Cu-labeled 1,4,8,11-tetraazacyclotetradecane-1,4,8,11-tetraacetic acid (^64^Cu-TETA) exhibit high uptake and retention in nontarget organs, which limits their application. Cross-bridged (CB) analogs, such as CB-DO2A ((1,4,7,10-tetraazabicyclo[5.5.2]tetradecane-4,10-diyl)diacetic acid), CB-TE2A ((1,4,8,11-tetraazabicyclo[6.6.2]hexadecane-4,11-diyl)diacetic acid), SarAr (1-N-(4-aminobenzyl)-3,6,10,13,16,19-hexa-aza-bicyclo-[6.6.6]eichosane-1,8-diamine), and NOTA (1,4,7-triazacyclononane-1,4,7-triacetic acid), demonstrate improved copper containment by enhancing the ligand's rigidity (2, 14).

Prasanphanich et al. recently reported that the NOTA-based ^64^Cu-NOTA-8-Aoc-BBN(7–14)NH_2_ (http://www.ncbi.nlm.nih.gov/books/NBK23504/) conjugate (where 8-Aoc = 8-aminooctanoic acid) exhibited decreased accumulation in hepatic tissue as compared with other chelator-based (DOTA, TETA, and CB-TE2A) conjugates (2, 14). To improve the tumor uptake and maintain the good pharmacokinetic properties of the ^64^Cu-NOTA-8-Aoc-BBN(7–14)NH_2_ conjugate, Lane et al. synthesized a new group of conjugates with the NOTA derivative NO2A and replaced the spacer 8-Aoc with an aliphatic or aromatic linking (1). These conjugates were abbreviated as ^64^Cu-NO2A-(X)-BBN(7–14)NH_2_, where X denotes the pharmacokinetic modifier, such as AMBA (para-aminobenzoic acid), β-Ala (beta-alanine), 5-Ava (5-aminovaleric acid), 6-Ahx, 8-Aoc, and 9-Anc (9-aminonanoic acid). The β-Ala, 5-Ava, 6-Ahx, and 9-Anc are aliphatic pharmacokinetic modifiers, ranging from three to nine carbons in length, whereas AMBA is an aromatic pharmacokinetic modifier and is more rigid than the aliphatic modifiers. Evidence indicates that a spacing moiety, ranging from three to eight carbons in length, can assist in receptor-mediated uptake (15). Conjugates containing an aromatic linker have significantly higher uptake and retention in PC-3 tumor tissue than those containing hydrocarbon or ether linkers (15, 16). Studies by Lane et al. have shown that the spacer X in the ^64^Cu-NO2A-(X)-BBN(7–14)NH_2_ conjugates has a significant role in clearance, accumulation, and retention of the conjugates in tumor tissue (1). The four conjugates showing the most favorable pharmacokinetic properties and the highest degree of pancreas and tumor accumulation were those in which X = 6-Ahx, 8-Aoc, 9-Anc, or AMBA. PET imaging with these conjugates produced high-contrast images of PC-3 tumor xenografts in severe combined immunodeficient (SCID) mice (1). This chapter describes the data obtained with ^64^Cu-NO2A-(6-Ahx)-BBN(7–14)NH_2_. Detailed information for other ^64^Cu-NO2A-(X)-BBN(7–14)NH_2_ conjugates is available in MICAD (http://www.ncbi.nlm.nih.gov/books/NBK5330/) (1).

### Related Resource Links:

- Protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&id=4885361), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nuccore&id=61677286) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=2925) information for GRPR
- Structure information of BN and analogs in PubChem (http://www.ncbi.nlm.nih.gov/pcsubstance/?term=bombesin)
- GRPR-targeted imaging agents in MICAD (http://www.ncbi.nlm.nih.gov/books/?term=GRPR%20AND%20micad%5bbook%5d)
- Chapter on ^64^Cu-NO2A-8-Aoc-BBN(7–14)NH_2_ (http://www.ncbi.nlm.nih.gov/books/NBK23504/) in MICAD

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=GRPR+and+bombesin+and+imaging+and+Smith)]

Lane et al. described the synthesis of ^64^Cu-NO2A-(X)-BBN(7–14)NH_2_ conjugates in detail (1). For ^64^Cu-NO2A-(6-Ahx)-BBN(7–14)NH_2_, the peptide 6-Ahx-BBN(7–14)NH_2_ was synthesized with traditional F-moc chemistry. Crude peptides were obtained in ~60% yield. NOTA was conjugated to the peptide via an active ester to produce the NOTA derivative conjugate, NO2A-(6-Ahx)-BBN(7–14)NH_2_, with ~80% yield after purification. The calculated and observed molecular weights for the NO2A-(6-Ahx)-BBN peptide conjugate were 1,338.7 and 1,338.8, respectively. ^64^Cu-NO2A-(6-Ahx)-BBN(7–14)NH_2_ was synthesized with the reaction of ^64^CuCl_2_ and peptide conjugate in the presence of ammonium acetate. The radiochemical yield was >90%. All of the unconjugated peptide precursors, peptide conjugates, and metallated peptide conjugates were purified with reverse-phase high-performance liquid chromatography (RP-HPLC) and characterized with mass spectrometry. The radiochemical purity and specific activity were not described.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=GRPR+and+bombesin+and+imaging+and+Smith)]

The stability of ^64^Cu-NO2A-(6-Ahx)-BBN(7–14)NH_2_ in human serum albumin was determined with quantification of the ^64^Cu-NO2A-(6-Ahx)-BBN(7–14)NH_2_ peak area in the radiometric RP-HPLC chromatogram. The percent of intact conjugate was >80% after 24 h incubation (37°C, 5% CO_2_-enriched atmosphere) with human serum albumin (1).

A competitive displacement binding assay was performed in PC-3 cells with ^125^I-(Tyr^4^)-BBN as the radioligand (1). High binding affinities were observed for both unlabeled NO2A-(6-Ahx)-BBN(7–14)NH_2_ (inhibition constant (K_i_) = 2.85 ± 0.15 nM) and ^nat^Cu-NO2A-(6-Ahx)-BBN(7–14)NH_2_ (^nat^Cu = natural copper) (K_i_ = 6.98 ± 1.99 nM).

Internalization was determined after incubation of the PC-3 cells with ^64^Cu-NO2A-(6-Ahx)-BBN(7–14)NH_2_ for different times. The percent of cell-associated radioactivity internalized after the 120-min incubation period was 4.8 ± 1.6%. Externalization was determined after an initial 40-min internalization period in PC-3 cells after which the cells were washed. The percent of ^64^Cu activity remaining internalized after 90 min of postincubation was 97.4 ± 4.5%. The results revealed GRPR-mediated trapping of radioactivity inside the cells (1).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=GRPR+and+bombesin+and+imaging+and+Smith)]

Biodistribution studies of ^64^Cu-NO2A-(6-Ahx)-BBN(7–14)NH_2_ were performed in both normal CF-1 mice (n = 4 or 5/group) and PC-3 xenograft-bearing SCID mice (n = 5 mice/group per time point). The biodistribution data were compared among the ^64^Cu-NO2A-(X)-BBN(7–14)NH_2_ conjugates (where X = β-Ala, 5-Ava, 6-Ahx, 8-Aoc, 9-Anc, or AMBA) (1, 2).

In normal mice, rapid clearance from blood was observed for all conjugates, with ≤0.5% injected dose per gram tissue (% ID/g) remaining in circulation at 1 h after injection (for ^64^Cu-NO2A-(6-Ahx)-BBN(7–14)NH_2_, 0.25 ± 0.06% ID/g). Excretion properties of the conjugates were directly related to the length of X. Increasing the hydrophobicity of the conjugate (increasing the aliphatic length of X) led to higher excretion rates via the hepatobiliary system. The hepatic accumulation for all conjugates at 1 h after injection ranged from 0.70% ID/g (where X = AMBA) to 2.35% ID/g (where X = 9-Anc), with 1.24 ± 0.19% ID/g for ^64^Cu-NO2A-(6-Ahx)-BBN(7–14)NH_2_. Uptake of the conjugates in GRPR-expressing pancreas ranged from 15.10 to 30.63% ID/g at 1 h after injection, with 26.87 ± 5.02% ID/g for ^64^Cu-NO2A-(6-Ahx)-BBN(7–14)NH_2_, indicating effective GRPR targeting for the radiolabeled conjugates. The four conjugates showing the most favorable pharmacokinetic properties and the highest degree of pancreas accumulation were those in which X = 6-Ahx, 8-Aoc, 9-Anc, or AMBA, which were further studied in PC-3 tumor-bearing SCID mice (1).

In tumor-bearing SCID mice, all four conjugates were cleared effectively from the bloodstream, with 0.93–1.35% ID/g remaining at 1 h after injection (for ^64^Cu-NO2A-(6-Ahx)-BBN(7–14)NH_2_, 1.20 ± 0.13% ID/g). Excretion routes were similar to those observed in normal CF-1 mice, with more hydrophobic conjugates excreted through the hepatobiliary system. Minimal accumulation of radioactivity was observed in the liver at 24 h, ranging from 0.68 to 1.37% ID/g (for ^64^Cu-NO2A-(6-Ahx)-BBN(7–14)NH_2_, 1.29 ± 0.08% ID/g), suggesting that the metal complex was effectively stable under in vivo conditions. High receptor-mediated accumulation was observed in both the pancreas and tumor for all conjugates. Radioactivity uptake values for ^64^Cu-NO2A-(6-Ahx)-BBN(7–14)NH_2_ at 1 h, 4 h, and 24 h after injection were 4.72 ± 0.59, 1.89 ± 0.31, and 1.14 ± 0.53% ID/g, respectively, in the tumor; 13.59 ± 1.81, 9.06 ± 0.91, and 2.19 ± 0.32% ID/g, respectively, in the pancreas; and 4.52 ± 0.41, 1.59 ± 0.15, and 1.29 ± 0.08% ID/g, respectively, in the kidney (1).

PET imaging was performed at 18 h after tail-vein injection of ^64^Cu-NO2A-(X)-BBN(7–14)NH_2_ (where X = 6-Ahx, 8-Aoc, 9-Anc, or AMBA) (1). The PC-3 tumors were clearly identifiable in PET images for all conjugates. Tumor/background ratios decreased with increased length of X, which appears to be a function of increasing the hydrophobicity of the conjugate. ^64^Cu-NO2A-(6-Ahx)-BBN(7–14)NH_2_ demonstrated high tumor uptake as well as relatively high kidney uptake. In comparison, for ^64^Cu-NO2A-(X)-BBN(7–14)NH_2_ where X = AMBA, superior tumor uptake with minimal liver accumulation was observed. For ^64^Cu-NO2A-(X)-BBN(7–14)NH_2_ where X = 8-Aoc, high tumor and liver uptake values were observed. For ^64^Cu-NO2A-(X)-BBN(7–14)NH_2_ where X = 9-Anc, moderate tumor uptake with significant abdominal accumulation (liver and gastrointestinal tract) was observed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20human)]

No references are currently available.

## References

1 Lane S.R., Nanda P., Rold T.L., Sieckman G.L., Figueroa S.D., Hoffman T.J., Jurisson S.S., Smith C.J. (2010). Optimization, biological evaluation and microPET imaging of copper-64-labeled bombesin agonists, [64Cu-NO2A-(X)-BBN(7-14)NH2], in a prostate tumor xenografted mouse model. Nucl Med Biol.
2 Prasanphanich A.F., Retzloff L., Lane S.R., Nanda P.K., Sieckman G.L., Rold T.L., Ma L., Figueroa S.D., Sublett S.V., Hoffman T.J., Smith C.J. (2009). In vitro and in vivo analysis of [(64)Cu-NO2A-8-Aoc-BBN(7-14)NH(2)]: a site-directed radiopharmaceutical for positron-emission tomography imaging of T-47D human breast cancer tumors. Nucl Med Biol.
3 Smith C.J., Volkert W.A., Hoffman T.J. (2003). Gastrin releasing peptide (GRP) receptor targeted radiopharmaceuticals: a concise update. Nucl Med Biol.
4 Erspamer V., Erpamer G.F., Inselvini M. (1970). Some pharmacological actions of alytesin and bombesin. J Pharm Pharmacol.
5 Ananias H.J., de Jong I.J., Dierckx R.A., van de Wiele C., Helfrich W., Elsinga P.H. (2008). Nuclear imaging of prostate cancer with gastrin-releasing-peptide-receptor targeted radiopharmaceuticals. Curr Pharm Des.
6 Schroeder R.P., van Weerden W.M., Bangma C., Krenning E.P., de Jong M. (2009). Peptide receptor imaging of prostate cancer with radiolabelled bombesin analogues. Methods.
7 Smith C.J., Volkert W.A., Hoffman T.J. (2005). Radiolabeled peptide conjugates for targeting of the bombesin receptor superfamily subtypes. Nucl Med Biol.
8 Zhang X., Cai W., Cao F., Schreibmann E., Wu Y., Wu J.C., Xing L., Chen X. (2006). 18F-labeled bombesin analogs for targeting GRP receptor-expressing prostate cancer. J Nucl Med.
9 Hohne A., Mu L., Honer M., Schubiger P.A., Ametamey S.M., Graham K., Stellfeld T., Borkowski S., Berndorff D., Klar U., Voigtmann U., Cyr J.E., Friebe M., Dinkelborg L., Srinivasan A. (2008). Synthesis, 18F-labeling, and in vitro and in vivo studies of bombesin peptides modified with silicon-based building blocks. Bioconjug Chem.
10 Mu L., Honer M., Becaud J., Martic M., Schubiger P.A., Ametamey S.M., Stellfeld T., Graham K., Borkowski S., Lehmann L., Dinkelborg L., Srinivasan A. (2010). In vitro and in vivo characterization of novel 18F-labeled bombesin analogues for targeting GRPR-positive tumors. Bioconjug Chem.
11 Becaud J., Mu L., Karramkam M., Schubiger P.A., Ametamey S.M., Graham K., Stellfeld T., Lehmann L., Borkowski S., Berndorff D., Dinkelborg L., Srinivasan A., Smits R., Koksch B. (2009). Direct one-step 18F-labeling of peptides via nucleophilic aromatic substitution. Bioconjug Chem.
12 Wadas T.J., Wong E.H., Weisman G.R., Anderson C.J. (2007). Copper chelation chemistry and its role in copper radiopharmaceuticals. Curr Pharm Des.
13 Hoffman T.J., Smith C.J. (2009). True radiotracers: Cu-64 targeting vectors based upon bombesin peptide. Nucl Med Biol.
14 Prasanphanich A.F., Nanda P.K., Rold T.L., Ma L., Lewis M.R., Garrison J.C., Hoffman T.J., Sieckman G.L., Figueroa S.D., Smith C.J. (2007). [64Cu-NOTA-8-Aoc-BBN(7-14)NH2] targeting vector for positron-emission tomography imaging of gastrin-releasing peptide receptor-expressing tissues. Proc Natl Acad Sci U S A.
15 Smith C.J., Gali H., Sieckman G.L., Higginbotham C., Volkert W.A., Hoffman T.J. (2003). Radiochemical investigations of (99m)Tc-N(3)S-X-BBN[7-14]NH(2): an in vitro/in vivo structure-activity relationship study where X = 0-, 3-, 5-, 8-, and 11-carbon tethering moieties. Bioconjug Chem.
16 Garrison J.C., Rold T.L., Sieckman G.L., Naz F., Sublett S.V., Figueroa S.D., Volkert W.A., Hoffman T.J. (2008). Evaluation of the pharmacokinetic effects of various linking group using the 111In-DOTA-X-BBN(7-14)NH2 structural paradigm in a prostate cancer model. Bioconjug Chem.